# ^99m^Tc-labeled anti-tumor necrosis factor-alpha monoclonal antibody

Chemical name: | ^99m^Tc-labeled anti-tumor necrosis factor-α monoclonal antibody
Abbreviated name: | ^99m^Tc-anti-TNF-α mAb
Synonym: | Remicade^®^
Agent Category: | Monoclonal antibody
Target: | Tumor necrosis factor-α
Target Category: | Antibody-ligand binding
Method of detection: | Single-photon emission computed tomography (SPECT) or gamma planar imaging
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click here for the protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=37210) and nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=158258710) sequence of TNF α.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+infliximab+human)]

The tumor necrosis factor alpha (TNF-α) is synthesized as a 26-kDa membrane-bound protein on certain cell types, e.g., T cells. The membrane-bound protein is cleaved to release a 17-kDa soluble form that exists as a homotrimer. It has been implicated in the pathogenesis of different diseases including cancer and inflammatory diseases such as rheumatoid arthritis (RA), Crohn’s disease (CD), and ulcerative colitis (1, 2). The stimulation of TNF-α induction is known to activate several pro-inflammatory cytokines, chemokines, matrix metalloproteinases, and endothelial adhesion molecules that attract cells known to promote inflammation (3). Because of its role in the pathogenesis of different inflammatory diseases, a variety of anti–TNF-α agents have been developed and investigated for the treatment of these conditions (4). Several anti–TNF-α antibodies such as infliximab, adalimumab, and certolizumab are now available for the treatment of TNF-α–mediated inflammatory diseases (2).

Infliximab is an anti–TNF-α, chimeric mouse-human IgG1 monoclonal antibody (mAb) that is commercially available and is approved (http://www.remicade.com/remicade/assets/Med_Guide.pdf) by the United States Food and Drug Administration for the treatment of a variety of inflammatory diseases (2, 4). This mAb is known to bind TNF-α in the serum or on the cell membranes and to inhibit its biological activity mediated through the TNF-α receptor. To evaluate its in vivo use for the detection of TNF-α in the various inflammatory diseases, infliximab was labeled with radioactive meta-stable technetium (^99m^Tc) and used as detailed below (2, 5-7).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(99m+Tc)+infliximab+synthesis)]

The ^99m^Tc labeling of infliximab was initiated by first reducing the mAb using the 2-mercaptoethanol (2-Me) method as described elsewhere (8). In brief, commercially available infliximab was dissolved in phosphate-buffered saline (PBS) and 2-Me was added to it in a 2-Me:infliximab ratio of 2,000:1 (5). The reaction was allowed to proceed for 30 min at room temperature, and the reduced antibody was purified on a Sephadex G25 column. The reduced antibody was aliquoted and stored in liquid nitrogen until required.

The methylene diphosphonate (MDP) bone scan kit (containing MDP, tin chloride, and ascorbic acid) was used for the labeling of infliximab (5). The MDP kit was reconstituted in saline, aliquoted, and stored at -20°C until necessary. The reconstituted MDP was added to the reduced infliximab and ^99m^Tc-labeled pertechnetate was added to the mixture. The solution was incubated at room temperature for 10 min and the preparation was analyzed by instant thin-layer chromatography to determine the labeling efficiency. The radiolabeled antibody had an Rf of 0, whereas pertechnetate and ^99m^Tc-labeled MDP had an Rf of 0.9–1.0. The labeling efficiency of the reaction was determined to be 98.2 ± 0.8%. The labeled antibody had a radiochemical purity of >95% as determined by high-performance liquid chromatography on a gel-filtration column. The specific activity of the labeled antibody was 2,775 ± 555 kBq/6.6 pmol (75 ± 15 µCi/6.6 pmol), and the radiotracer was determined to be stable for up to 8 h in human serum or saline.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(99m+Tc)+infliximab+in+vitro)]

The binding characteristics of labeled infliximab were determined with a competitive binding assay using human lymphocytes (5). Induction of membrane-bound TNF-α was carried out by exposure of the cells to phytohemagglutinin. The cells expressing TNF-α were then exposed either to an increasing concentration of ^99m^Tc-labeled infliximab alone or [^99m^Tc]infliximab in the presence of a molar excess of unlabeled antibody. A competitive, dose-dependent inhibition of [^99m^Tc]-infliximab by the unlabeled antibody was observed. The labeled antibody had a dissociation constant (K_d_) of 4.67 × 10^-10^ M for TNF-α on the stimulated lymphocytes.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(99m+Tc)+infliximab+rodentia)]

The use of [^99m^Tc]-infliximab as an inflammation imaging agent was evaluated and compared to ^99m^Tc-tin colloid–labeled leukocytes in a rat colitis model (6). Uptake ratios of 2.7 ± 1.0 and 2.6 ± 0.3 were observed in the inflamed colon at 1 and 4 h, respectively, after the administration of [^99m^Tc]-infliximab. The labeled leukocytes yielded ratios of 19.5 ± 9.9 and 41.2 ± 16.1 at 1 and 4 h, respectively. The investigators suggested that although the uptake was lower for [^99m^Tc]-infliximab, the labeled antibody can be used for imaging inflammatory bowel disease in humans because it is easy to prepare compared to the labeled leukocytes (6).

The biodistribution of [^99m^Tc]-infliximab was investigated in mice (5). The labeled antibody showed a slow clearance from the blood and had a mixed hepatic/renal metabolism with little accumulation over 24 h in the gut of the animals. Similar pharmacokinetics have also been observed with other labeled antibodies (9).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(99mTc)+infliximab+non-primate+mammals)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(99mTc)+infliximab+non-human+primates)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+infliximab+human)]

Imaging studies of CD patients treated with ^99m^Tc-infliximab showed renal accumulation of the label immediately after the treatment, and the radioactivity was cleared from blood circulation by ~6 h (5). For comparison the patients were also treated with ^99m^Tc-labeled hexamethylpropyleneamine oxime (HMPAO) autologous white blood cells. Bowel uptake of the radioactivity was reported in 6 of the 10 treated patients. With the [^99m^Tc]-HMPAO-labeled leukocytes, 8 of 10 patients were positive for the label. The investigators observed that the 6 patients positive for [^99m^Tc]-infliximab showed a lower accumulation of the label compared to the accumulation of labeled leukocytes.

An increased level of TNF-α has been reported in the inflamed joints of individuals suffering from synovial inflammation, and the use of intra-articular infliximab was reported to be beneficial for the treatment of RA, ankylosing spondylitis, and Behçet’s disease (10-12). Conti et al. used an in vivo injection of [^99m^Tc]-infliximab to assess the expression of TNF-α in the arthritic knee of an individual (13). The investigators observed an accumulation of the label in the affected knee, indicating that an increased level of TNF-α was present in the joint. They removed the synovial fluid from the knee and injected a single bolus of cold infliximab, which resulted in complete remission of the arthritis. After complete remission the patient was given another injection of labeled infliximab and evaluated by scintigraphy for the accumulation of the label. No radioactivity was detected in the knee joint, indicating the absence of TNF-α . From these observations the investigators suggested this approach could be used to screen patients for intra-articular infliximab therapy (13).

In another study, van der Laken et al. investigated the development of anti-infliximab antibodies in patients with RA who did not respond to infliximab therapy (7). For this the investigators infused infliximab responders and infliximab non-responders with [^99m^Tc]-infliximab. By planar gamma imaging they observed lower whole-body retention of the label (76% of injected dose) in the non-responders compared to the responders (98–100% of the injected dose) at 24 h after the injection. Compared to responders, the label was observed to accumulate in the liver, spleen, and inflamed joints of the non-responding individuals. Using a sucrose density gradient, the serum of non-responders was observed to possibly contain infliximab-IgG complexes that were absent in the serum obtained from the responding individuals (7). The investigators suggested that the non-responders had probably developed anti-infliximab antibodies that bound to infliximab and were taken up by the liver.

## References

1 Maisey N. (2007). Antitumor Necrosis Factor (TNF-a) Antibodies in the Treatment of Renal Cell Cancer. Cancer Invest.
2 Tilg H., Moschen A., Kaser A. (2007). Mode of function of biological anti-TNF agents in the treatment of inflammatory bowel diseases. Expert Opin Biol Ther.
3 Locksley R.M., Killeen N., Lenardo M.J. (2001). The TNF and TNF receptor superfamilies: integrating mammalian biology. Cell.
4 Kooloos W.M., de Jong D.J., Huizinga T.W., Guchelaar H.J. (2007). Potential role of pharmacogenetics in anti-TNF treatment of rheumatoid arthritis and Crohn's disease. Drug Discov Today.
5. D'Alessandria, C., G. Malviya, A. Viscido, A. Aratari, F. Maccioni, A. Amato, F. Scopinaro, R. Caprilli, and A. Signore, Use of a (99m)Tc labeled anti-TNFalpha monoclonal antibody in Crohn's disease: in vitro and in vivo studies. Q J Nucl Med Mol Imaging, 2007.
6 Tsopelas C., Penglis S., Ruskiewicz A., Bartholomeusz D.L. (2006). Scintigraphic imaging of experimental colitis with technetium-99m-infliximab in the rat. Hell J Nucl Med.
7 van der Laken C.J., Voskuyl A.E., Roos J.C., Stigter van Walsum M., de Groot E.R., Wolbink G., Dijkmans B.A., Aarden L.A. (2007). Imaging and serum analysis of immune complex formation of radiolabelled infliximab and anti-infliximab in responders and non-responders to therapy for rheumatoid arthritis. Ann Rheum Dis.
8 Mather S.J., Ellison D. (1990). Reduction-mediated technetium-99m labeling of monoclonal antibodies. J Nucl Med.
9 Chianelli M., Parisella M.G., D'Alessandria C., Corsetti F., Scopinaro F., Signore A. (2003). The developing role of peptide radiopharmaceuticals in the study of chronic inflammation: new techniques for novel therapeutic options. Q J Nucl Med.
10 Partsch G., Wagner E., Leeb B.F., Dunky A., Steiner G., Smolen J.S. (1998). Upregulation of cytokine receptors sTNF-R55, sTNF-R75, and sIL-2R in psoriatic arthritis synovial fluid. J Rheumatol.
11 Andonopoulos A.P. Meimaris N. Daoussis D. Bounas A. Yiannopoulos G. Intra-articular anti-tumor necrosis factor alpha antibody in recalcitrant arthritis of Behcet's disease Clin Exp Rheumatol 2003 21 Suppl 30 4 S57 8 14727465
12 Nikas S.N., Temekonidis T.I., Zikou A.K., Argyropoulou M.I., Efremidis S., Drosos A.A. (2004). Treatment of resistant rheumatoid arthritis by intra-articular infliximab injections: a pilot study. Ann Rheum Dis.
13 Conti F., Priori R., Chimenti M.S., Coari G., Annovazzi A., Valesini G., Signore A. (2005). Successful treatment with intraarticular infliximab for resistant knee monarthritis in a patient with spondylarthropathy: a role for scintigraphy with 99mTc-infliximab. Arthritis Rheum.